# ImPyβImPyβImβ-C_3_-^18^F

Chemical name: | ImPyβImPyβImβ-C_3_-^18^F
Abbreviated name: | [^18^F]PIPAM5
Synonym:
Agent category: | Macromolecule
Target: | DNA
Target category: | Nucleic acid binding molecule
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is current available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=5-ring b-linked polyamides +18F)]

Polyamides (PAM) constructed from N-methylpyrrole (Py), N-methylimidazole (Im), 3-chlorothiophene (Ct), and N-methylhydroxypyrrole (Hp) amino acids comprise a class of synthetic oligomeric ligands that bind to the minor groove of DNA (1, 2). The aromatic heterocycles in the PAM orientate antiparallel with respect to the Watson-Crick base pair (bp), which leads to a specific recognition of DNA sequences (3). The recognition process follows a series of pairing rules; i.e., an ImPy specifies for G·C, a PyPy binds both A·T and T·A, an HpPy discriminates T·A over A·T, and a CtPy prefers T·A over A·T at the N-terminus. These aromatic amino acids can be programmed to a strand with more than two residues to recognize longer DNA sequences; for example, an ImPyPy motif specifies for the five-bp sequence 5’-WGWCW-3’ (W=A, T) instead of 5’-WGWWW-3’ (4). More complicated PAM motifs can be designed by adding small molecules such as β-alanine or γ-aminobutyric acid to covalently link between two antiparallel PAM strands, yielding substantial increases in affinities and specificities. For instance, an eight-ring hairpin motif, which has a γ-aminobutyric acid (γ-turn) linker to connect the carboxylic terminus of one polyamide to the amino terminus of another, exhibits ~100-fold higher affinity for binding a six-bp DNA sequence compared to the unlinked homodimers (4). PAM are molecules that can permeate cell membranes and have been used in targeting a variety of DNA sequences in cell culture (5). The binding of PAM replaces the DNA-binding proteins and thus regulates the transcription of selected genes. The use of radiolabeled PAM aims at imaging gene regulations in vivo.

Fluorine-18 [^18^F], with a half-life of 109.7 min and low β^+^-energy (0.64 MeV), represents the ideal radionuclide for position emission tomography (PET). The ^18^F-produced positron is annihilated with an electron, leading to the emission of two 511-keV photons ~180º apart, which is detected coincidentally with PET. Various peptides have been successively fluorinated with multistep ^18^F-acylation, using ^18^F-labeled prosthetic groups such as amino-reactive ^18^F-labeling agent N-succinimidyl 4-[^18^F]fluorobenzoate (6). To increase labeling efficiency, the fluorination also can be conducted via a two-step synthetic approach in which an oxime is formed between an aminooxy group in the peptide and an ^18^F-labeled aldehyde such as 4-[^18^F]fluorobenzaldehyde (6). ImPyβImPyβImβ-C_3_-^18^F ([^18^F]PIPAM5) is an ^18^F-labeled PAM used for PET that is obtained with the oxime ligation approach (5). [^18^F]PIPAM5 contains five aromatic amino acids connected with β-alanine, which is denoted as β and is also known as a five-ring β-linked motif. Its unlabeled form with an N-N-dimethylaminopropyl tail has been exhibit ability to upregulate the repressed gene frataxin in a cell culture mode of Friedreich’s ataxia (7).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(5-ring b-linked polyamides +18F)+AND+synthesis%0D%0A)]

Harki et al. reported the synthesis of [^18^F]PIPAM5 (5). Initially, 4-[^18^F]-fluorobenzaldehyde was obtained by nucleophilic fluorination of a trimethylammonium benzaldehyde derivative with cyclotron-produced [^18^F]fluoride in the presence of 5,6-benzo-4,7,13,16,21,24-hexaoxa-1,10-diazabicyclo[8.8.8]hexacos-5-ene (Kryptofix[2.2.2]). The β-linked PAM ImPyβImPyβImβ was synthesized on a Boc-β-alanine phenylacetamidomethyl resin according to standard protocols. Then the PAM was hydroxylamine-functionalized in DMF by reaction with tert-butyl-3-aminopropoxycarbamate in the presence of benzotriazolyloxy-tris-(pyrrolidino)-phosphonium hexafluorophosphate (PyBOP) and N,N,-diisopropylethylamine. Finally, the obtained ImPyβImPyβImβ-hydroxylamine was ligated with the 4-[^18^F]-fluorobenzaldehyde with aniline as a catalyst to produce [^18^F]PIPAM5 at radiochemical yield of 12%. The whole synthetic procedure was completed in 100 min after the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(5-ring b-linked polyamides +18F)+AND+%22in+vitro%22)]

Harki et al. used the cold PAM analog [^19^F]PIPAM5 to evaluate its affinity to DNA in vitro (5). Quantitative DNaseI footprint titrations were performed on the 5’-^32^P-polymerase chain reaction fragment from plasmid pJWP-16. In this method, equilibrium mixtures of ^32^P end-labeled DNA and a range of PAM concentrations were partially digested by DNase I followed by gel electrophoresis and autoradiography. The PAM bound DNA was protected from cleavage, which produced a band gap on the gel. Quantification of the binding fraction as a function of PAM concentration was used to the apparent association constant, 3.5 ± 2.1 × 10^9^ M^-1^ for [^19^F]PIPAM5.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(5-ring b-linked polyamides +18F) +AND++rodentia)]

Harki et al. examined the biodistribution of [^18^F]PIPAM5 in vivo by PET and computed tomography (CT) (5). C57 mice were injected intravenously with [^18^F]PIPAM5 at doses of 472, 218, and 193 μCi (17.5, 8.06 and 7.141 MBq), respectively, and PET images were collected for 2 to 3 h. At 4 min after injection, ~46% of injected [^18^F]PIPAM5 was found in the liver. At 20 min after injection, 35% to 40% of injected [^18^F]PIPAM5 was observed in the gastrointestinal tract and maintained a constant for the entire PET scan. No significant radioactivity was found in the brain, heart, or bone. Thus, the clearance of [^18^F]PIPAM5 was primarily via the liver by excretion through the gallbladder and entry into small intestine; the renal clearance was <1.5%.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(5-ring b-linked polyamides +18F) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(5-ring b-linked polyamides +18F) +AND+human)]

No publication is currently available.

### NIH Support

GM 27681, EB 01943, CA 92865

## References

1 Hsu C.F., Phillips J.W., Trauger J.W., Farkas M.E., Belitsky J.M., Heckel A., Olenyuk B.Z., Puckett J.W., Wang C.C., Dervan P.B. (2007). Completion of a Programmable DNA-Binding Small Molecule Library. Tetrahedron.
2 Nickols N.G., Jacobs C.S., Farkas M.E., Dervan P.B. (2007). Improved nuclear localization of DNA-binding polyamides. Nucleic Acids Res.
3 Belitsky J.M., Nguyen D.H., Wurtz N.R., Dervan P.B. (2002). Solid-phase synthesis of DNA binding polyamides on oxime resin. Bioorg Med Chem.
4 Dervan P.B., Edelson B.S. (2003). Recognition of the DNA minor groove by pyrrole-imidazole polyamides. Curr Opin Struct Biol.
5 Harki D.A., Satyamurthy N., Stout D.B., Phelps M.E., Dervan P.B. (2008). In vivo imaging of pyrrole-imidazole polyamides with positron emission tomography. Proc Natl Acad Sci U S A.
6 Poethko T., Schottelius M., Thumshirn G., Hersel U., Herz M., Henriksen G., Kessler H., Schwaiger M., Wester H.J. (2004). Two-step methodology for high-yield routine radiohalogenation of peptides: (18)F-labeled RGD and octreotide analogs. J Nucl Med.
7 Burnett R., Melander C., Puckett J.W., Son L.S., Wells R.D., Dervan P.B., Gottesfeld J.M. (2006). DNA sequence-specific polyamides alleviate transcription inhibition associated with long GAA.TTC repeats in Friedreich's ataxia. Proc Natl Acad Sci U S A.